# Sialy Lewis^x^ mimetic conjugated to pegylated ultrasmall superparamagnetic iron oxide nanoparticles

Chemical name: | Sialy Lewis^x^ mimetic conjugated to pegylated ultrasmall superparamagnetic iron oxide nanoparticles
Abbreviated name: | USPIO-PEG-sLeX
Synonym:
Agent category: | Compound
Target: | E-selectin
Target category: | Adhesion molecule
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=34420911), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4506870) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6401) for more information about E-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

USPIO is composed of iron nanoparticles of 4–6 nm diameters and the hydrodynamic diameter with dextran or polyethylene glycol (PEG) coating is 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life is calculated to be ~24 h in humans (2) and 2 h in mice (3). Because of its long blood half-life, USPIO can be used as blood pool agent during the early phase of intravenous administration (4). In the late phase, USPIO is suitable for the evaluation of RES in the body, particularly in lymph nodes (5). E-selectin is found on the cell surface of endothelial cells (6, 7). It binds to sialy-Lewis^x^ (a carbohydrate moiety) on the cell-surface of leukocytes. Tumor necrosis factor α (TNFα) and interleukin-1 (IL-1), released from inflammatory stimuli, upregulate E-selectin and other adhesion molecule expression on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium. A sialy-Lewis^x^ mimetic (sLeX) was conjugated to USPIO (USPIO-g-sLeX) nanoparticles for non-invasive MRI of E-selectin expression on activated endothelial cells (8). Radermacher et al. (9) coupled sLeX on USPIO coated with hydrophilic polyethylene glycol (PEG) to improve blood circulation time and minimize the non-specific binding of USPIO to tissues. USPIO-PEG-sLeX has been studied for in vivo imaging of inflamed tissues in mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (E-selectin (http://www.ncbi.nlm.nih.gov/gene/6401)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D)
- Drug information in FDA (E-selectin (http://google2.fda.gov/search?q=e-selectin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20synthesis)]

A solution of sialy-Lewis^x^ mimetic (10 mg) and N-(3-dimethylaminopropyl)-N’-ethylcarbodiimide hydrochloride (6 mg) was added to USPIO nanoparticles and stirred at room temperature for 20 h (9). The nanoparticle mixture was ultrafiltered on a 30-kD membrane and mixed with a solution of aminoPEG750 and ethylcarbodiimide hydrochloride at room temperature for 17 h. USPIO-PEG-sLeX nanoparticles were purified with ultrafiltration. USPIO-PEG-sLeX nanoparticles had a hydrodynamic size of 23 nm in diameter. USPIO-PEG-sLeX exhibited r_1_ and r_2_ relaxivity values of 15.4 and 87.8 mM^-1^ s^-1^ at 60 MHz and 37ºC, respectively. The number of sLeX molecules per nanoparticle was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20in%20vitro)]

Boutry et al. (8) performed in vitro binding studies of USPIO-g-sLeX and USPIO in cultured human umbilical vein endothelial cells (HUVECs) with T2-weighted MRI. HUVECs were stimulated with TNFα and incubated with 4 mM USPIO-g-sLeX or USPIO for 1 h, which showed extensive retention of USPIO-g-sLeX on TNFα-stimulated HUVECs. Image intensity and R_2_ measurements performed on T2-weighted MR images demonstrated a significantly higher (P<0.01) negative enhancement of USPIO-g-sLeX than USPIO on stimulated HUVECs and on non-stimulated HUVECs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20rodentia)]

Inflammation was induced on the right rear legs of mice by intramuscular injection of Freund’s complete adjuvant (FCA) (9). USPIO-PEG-sLeX or USPIO-PEG (7.7 mg Fe/kg) were injected intravenously in the mice (n = 5-6 mice/group) at 24 h after FCA injection. T2-weighted MR images (4.7 T) of the legs were obtained at 0.5-3 h after injection. There was a loss of signal intensity of 49 ± 4% and 54 ± 4% for USPIO-PEG-sLeX at 1 and 3 h after injection, respectively. The loss was less pronounced with USPIO-PEG (36 ± 4%) at 3 h. There was also a 10% loss of signal intensity in the control muscle after injection of both nanoparticles. The mean changes in T2 values were 41.8 ms for USPIO-PEG-sLeX and 21.1 ms for USPIO-PEG (P <0.05). EX vivo biodistribution of the nanoparticles were measured with electron paramagnetic resonance (ESR) spectroscopy. USPIO-PEG-sLeX and USPIO-PEG accumulated quickly in macrophages in the liver and spleen. Both nanoparticles were not detected in the blood at 24 h with ~18% and 3% of the initial blood concentration at 1h and 6 h after injection, respectively. The tissues with the highest Fe accumulation were the spleen and liver at 3 h after injection. The amount of Fe in the inflamed muscle was 5 and 2 fold greater than the control muscle for USPIO-PEG-sLeX and USPIO-PEG, respectively. The amount of Fe accumulation in the inflamed muscle was 0.8% of injected dos (ID) for USPIO-PEG-sLeX and 0.4% ID for USPIO-PEG. ESR imaging of the inflamed tissues in mice in vivo showed about 1-fold higher signal intensity with USPIO-PEG-sLeX than with USPIO-PEG. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
4 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
5 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
6 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
7 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
8 Boutry S., Laurent S., Elst L.V., Muller R.N. (2006). Specific E-selectin targeting with a superparamagnetic MRI contrast agent. Contrast Media Mol Imaging.
9 Radermacher K.A., Beghein N., Boutry S., Laurent S., Vander Elst L., Muller R.N., Jordan B.F., Gallez B. (2009). In vivo detection of inflammation using pegylated iron oxide particles targeted at E-selectin: a multimodal approach using MR imaging and EPR spectroscopy. Invest Radiol.